# Indocyanine green–enhanced, cyclic Arg-Gly-Asp–conjugated, PEGylated single-walled carbon nanotubes

Chemical name: | Indocyanine green–enhanced, cyclic Arg-Gly-Asp–conjugated, PEGylated single-walled carbon nanotubes
Abbreviated name: | SWNT-ICG-RGD
Synonym:
Agent Category: | Nanoparticles
Target: | Integrin α_v_β_3_
Target Category: | Receptor
Method of detection: | Ultrasound, Photoacoustic Imaging (PAI)
Source of signal / contrast: | Indocyanine green (ICG)
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=photoacoustic+imaging)]

Photoacoustic imaging (PAI) is a hybrid imaging modality based on the photoacoustic effect where absorption of electromagnetic energy (non-ionizing laser or radio-frequency pulses) is converted into ultrasound waves that are detected outside the subject of interest (1-4). It takes advantage of sensitive optical absorption contrast and low acoustic scattering (two to three orders of magnitude weaker for ultrasound than for optical scattering) in soft tissue. The PAI signal from the photoacoustic effect is proportional to the local optical absorption and thus contains functional and molecular information about the target of interest (3, 5). In addition, PAI can achieve better than submillimeter resolution in centimeters of depth (4). At the same time, PAI inherits some limitations from both acoustic and electromagnetic radiation, such as strong ultrasonic wave aberration from hard tissues, contact measurement, and light attenuation from light scattering (1, 6).

Currently, two types of PAI systems, photoacoustic tomography and photoacoustic microscopy, have been developed for angiogenesis visualization, tumor detection, blood oxygenation mapping, and functional brain imaging (5, 7-10). However, some pathological lesions fail to generate sufficient photoacoustic contrast and require an exogenous agent to enhance the absorption contrast for detection (1, 11). Nanoparticles have been synthesized as PAI contrast agents on the basis of either their surface plasmon resonance or the near-infrared fluorescent dyes they can carry (1, 6, 11). The near-infrared optical window allows light to penetrate up to several centimeters into biological tissues, and the optical properties of tissues within this region are closely related to the tissue's molecular constituents. Challenges remain with respect to producing sufficient photoacoustic signal with low concentrations of contrast agents (2, 4).

de la Zerda et al. developed a targeted nanoparticle probe by conjugating cyclic Arg-Gly-Asp (RGD) peptides to PEGylated single-walled carbon nanotubes (SWNTs) for α_v_β_3_ integrin targeting and attaching indocyanine green (ICG) dye to the surface of nanotubes for absorption contrast enhancement (referred to as SWNT-ICG-RGD) (1). The ultrahigh surface area of nanotubes allows highly efficient loading of ICG on the nanotube surface. SWNT-ICG-RGD have been characterized in vitro and tested in animal tumor models (1).

### Related Resource Links:

- MICAD chapters on SWNT-related agents (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=single-walled+carbon+nanotubes++AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Protein information of integrin α_v_β_3_ (http://www.ncbi.nlm.nih.gov/protein/?term=Integrin+%CE%B1v%CE%B23)
- Articles about integrins in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Integrin%20%CE%B1v%CE%B23)
- MICAD chapters on integrins (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=integrin+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20499887)]

Synthesis of the cyclic RGD peptide–conjugated and PEGylated SWNTs (RGD-PEG-SWNTs or SWNT-RGD) has been described previously by Liu et al., and relevant data obtained from RGD-PEG-SWNTs have been introduced in the MICAD chapter on RGD-PEG-SWNTs (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=RGDSWNTs) (12). de la Zerda et al. attached ICG dye to the surface of RGD-PEG-SWNTs with overnight incubation to generate ICG-enhanced RGD-PEG-SWNTs (SWNT-ICG-RGD) (1). Unbound ICG molecules were removed with filtration through 100-kDa centrifuge filters. The SWNTs used in this study were 50–300 nm in length and 1–2 nm in diameter. The molar concentrations of SWNTs used in the synthesis were calculated on the basis of an average molecular weight of 170 kDa per SWNT (150 nm in length and 1.2 nm in diameter). Control nanoparticles (SWNT-ICG-RAD) were also synthesized with a mutated nontargeted peptide, RAD, instead of RGD. The purity, ICG labeling efficiency, and yield of the nanoparticles were not described in detail.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20499887)]

The stability of SWNT-ICG-RGD (peak optical absorbance: 780 nm) in serum was evaluated after incubation of the SWNT-ICG-RGD with 10% serum and after exposure to a 780-nm laser at a power density of 8 mJ/cm^2^ (the power density used in animal experiments) (1). SWNT-ICG-RGD showed steady optical absorption in serum over 24 h of incubation. The absorbance standard deviation in serum through the entire 24 h was within 2% of the average, and the maximum deviation from average was <7%. Exposure of SWNT-ICG-RGD to laser light resulted in a 30% loss of the optical absorbance after 60 min of irradiation, exhibiting good resistance to photobleaching.

In vitro targeting capability of SWNT-ICG-RGD was studied after incubation of the nanoparticles with cultured U87MG (human glioblastoma) cells for 30 min to 4 h. Cells exposed to SWNT-ICG-RGD had greater absorbance than cells exposed to control SWNT-ICG-RAD (P < 0.05 for all time points). At 1 h and 2 h of incubation, the optical absorption was approximately two-fold higher for cells exposed to SWNT-ICG-RGD than for cells exposed to SWNT-ICG-RAD, suggesting specific binding of SWNT-ICG-RGD to the α_v_β_3_ receptor. Blocking studies were not performed (1).

The photoacoustic signal linearity as a function of agent concentrations was tested with a non-scattering and non-absorbing agar-phantom (1). SWNT-ICG-RGD particles were embedded 2–3 mm deep in the agar phantom. The photoacoustic signal produced by the particles was closely correlated with the particle concentration (R^2^ = 0.983).

Comparison between plain RGD-PEG-SWNTs and ICG-enhanced SWNT-ICG-RGD was performed after incubation of the nanoparticles with cultured U87MG cells (expressing α_v_β_3_ integrin) for 2 h. Cells were collected and embedded in a clear agarose phantom. PAI showed that cells exposed to SWNT-ICG-RGD were detected at concentrations 20 times lower than the concentrations of cells exposed to plain RGD-PEG-SWNTs (P < 0.0001), which was consistent with the optical absorbance of SWNT-ICG-RGD being ~20 times higher than plain RGD-PEG-SWNTs (1, 12).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20499887)]

Nanoparticle sensitivity in mice was tested after subcutaneous injection of SWNT-ICG-RAD (instead of SWNT-ICG-RGD) mixed with matrigel into the lower back of mice (n = 3) (1). SWNT-ICG-RAD had similar optical spectrum as SWNT-ICG-RGD. SWNT-ICG-RAD produced significant photoacoustic contrast, while matrigel alone did not. There was a linear correlation between the SWNT-ICG-RAD concentration and the corresponding photoacoustic signal (R^2^ = 0.97). SWNT-ICG-RAD at 170 pmol generated a photoacoustic signal equivalent to that of the tissue background (i.e., signal/background ratio = 1).

PAI of tumors was performed after tail vein injection of either SWNT-ICG-RGD (targeted) or SWNT-ICG-RAD (untargeted control) to mouse bearing U87MG tumor xenografts (n = 4 mice/group). Mice injected with SWNT-ICG-RGD showed significantly higher photoacoustic signal in the tumor compared with the control group injected with SWNT-ICG-RAD (P < 0.001). At 2 h after injection, the photoacoustic signal in the tumor was >100% higher for mice injected with SWNT-ICG-RGD than for mice injected with SWNT-ICG-RAD (1). No blocking studies were carried out.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 de la Zerda A., Liu Z., Bodapati S., Teed R., Vaithilingam S., Khuri-Yakub B.T., Chen X., Dai H., Gambhir S.S. (2010). Ultrahigh sensitivity carbon nanotube agents for photoacoustic molecular imaging in living mice. Nano Lett.
2 Yang X., Stein E.W., Ashkenazi S., Wang L.V. (2009). Nanoparticles for photoacoustic imaging. Wiley Interdiscip Rev Nanomed Nanobiotechnol.
3 Hu S., Wang L.V. (2010). Photoacoustic imaging and characterization of the microvasculature. J Biomed Opt.
4 Wang L.V. (2008). Prospects of photoacoustic tomography. Med Phys.
5 Zhang H.F., Maslov K., Stoica G., Wang L.V. (2006). Functional photoacoustic microscopy for high-resolution and noninvasive in vivo imaging. Nat Biotechnol.
6 de la Zerda A., Zavaleta C., Keren S., Vaithilingam S., Bodapati S., Liu Z., Levi J., Smith B.R., Ma T.J., Oralkan O., Cheng Z., Chen X., Dai H., Khuri-Yakub B.T., Gambhir S.S. (2008). Carbon nanotubes as photoacoustic molecular imaging agents in living mice. Nat Nanotechnol.
7 Oh J.T., Li M.L., Zhang H.F., Maslov K., Stoica G., Wang L.V. (2006). Three-dimensional imaging of skin melanoma in vivo by dual-wavelength photoacoustic microscopy. J Biomed Opt.
8 Song K.H., Stein E.W., Margenthaler J.A., Wang L.V. (2008). Noninvasive photoacoustic identification of sentinel lymph nodes containing methylene blue in vivo in a rat model. J Biomed Opt.
9 Song K.H., Stoica G., Wang L.V. (2006). In vivo three-dimensional photoacoustic tomography of a whole mouse head. Opt Lett.
10 Wang X., Xie X., Ku G., Wang L.V., Stoica G. (2006). Noninvasive imaging of hemoglobin concentration and oxygenation in the rat brain using high-resolution photoacoustic tomography. J Biomed Opt.
11 Zhang Q., Iwakuma N., Sharma P., Moudgil B.M., Wu C., McNeill J., Jiang H., Grobmyer S.R. (2009). Gold nanoparticles as a contrast agent for in vivo tumor imaging with photoacoustic tomography. Nanotechnology.
12 Liu Z., Cai W., He L., Nakayama N., Chen K., Sun X., Chen X., Dai H. (2007). In vivo biodistribution and highly efficient tumour targeting of carbon nanotubes in mice. Nat Nanotechnol.